# Hyaluronan conjugated with IR-783

Chemical name: | Hyaluronan conjugated with IR-783
Abbreviated name: | IR783-HA
Synonym:
Agent category: | Glycosaminoglycan
Target: | Lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1)
Target category: | Receptor
Method of detection: | Optical, fluorescence imaging
Source of signal/contrast: | IR-783
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LYVE-1)]

The primary function of the lymphatic system is to drain ~10% of the interstitial fluid from small capillaries to lymphatic vessels through lymph nodes (LNs) and finally to the venous system (1-5). LNs form a natural filter for lymphatic drainage and prevent the possible migration of cancer cells from the lymphatic system into the rest of the body. As the first LN that receives lymph drainage from a tumor bed, the sentinel LN is very likely to contain cancer cells if the primary tumor has spread via the lymphatic system (1, 2). The lymphatic system is complex, and its detection and mapping remain challenging (1, 2, 6, 7). However, with advances of new imaging agents and techniques, imaging and mapping of both the lymphatic vessels and the LNs are now possible with x-ray–computed tomography, ultrasound, nuclear medicine, and magnetic resonance imaging (7-9). There is increasing evidence that tumor cells induce lymphangiogenesis in tumor-draining LNs in experimental models of cancer (10, 11) as well as in LNs of patients with metastatic melanoma and breast cancer (12, 13). Therefore, LN lymphangiogenesis might provide a target to image the early stages of tumor metastasis. In addition, chronic inflamed tissues produce vascular endothelial growth factor to induce lymphangiogenesis in draining LNs.

Hyaluronan (HA) is an abundant extracellular matrix glycosaminoglycan in skin and mesenchymal tissues, where it facilitates cell migration during inflammation, wound healing, metastasis, and embryonic morphogenesis (14, 15). CD44 is an integral cell membrane glycoprotein on leukocytes and has an important role in matrix adhesion, lymphocyte activation, and leukocyte LN homing (16). CD44 binds HA to induce extravasation of lymphoid cells. Lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1) has a 41% homology to CD44, and LYVE-1 expression is largely restricted to endothelial cells of lymphatic vessels and splenic sinusoidal endothelial cells. Expression is undetectable on lymphocytes, hematopoietic cells, or vascular endothelial cells. Among various near-infrared agents, only indocyanine green (ICG), with absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (17). Sharma et al. (18) conjugated HA with near-infrared dye IR-783 to form IR783-HA for imaging of the lymphatic vasculature in pigs.

### Related Resource Links:

- Chapters in MICAD (LYVE-1 (http://www.ncbi.nlm.nih.gov/books?term=LYVE-1%20AND%20micad%5Bbook%5D), CD44 (http://www.ncbi.nlm.nih.gov/books?term=CD44%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (LYVE-1 (http://www.ncbi.nlm.nih.gov/gene/10894), CD44 (http://www.ncbi.nlm.nih.gov/gene/960))
- Articles in Online Mendelian Inheritance in Man (OMIM) (LYVE-1 (http://www.ncbi.nlm.nih.gov/omim/605702), CD44 (http://www.ncbi.nlm.nih.gov/omim/107269))
- Clinical trials (LYVE-1 (http://www.clinicaltrials.gov/ct2/show/NCT00748657?term=LYVE1&rank=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20hyaluronan%20AND+synthesis)]

IR783-HA was prepared by conjugation of IR-783 to HA through a hexane-1,-6-diamine linkage (18). IR783-HA consisted of 2 molar percent IR-783. IR-783 has an extinction of coefficient of 157,000 M^-1^cm^-1^ and a quantum yield of 0.11, with a maximal excitation wavelength of 768 nm and a maximal emission wavelength of 784 nm in saline.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20hyaluronan%20AND+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20hyaluronan+AND+rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20hyaluronan+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

Sharma et al. (18) performed real-time imaging of lymphatic vessels with IR783-HA using a small-animal fluorescence imaging system. Intradermal injection of IR783-HA was performed in the swine hind limb vessel (n = 4). IR783-HA uniformly demarcated the lymphatic vessel wall and LNs during 4 h of imaging. In contrast, ICG showed propulsion of packets of ICG fluorescence with fluctuation and reduction of intensity along the lymphatic vessel as a function of time. These observations were consistent with the binding of IR783-HA and non-binding of ICG to LYVE-1 present on the lymphatic endothelium. No blocking studies were carried out to show binding to the LYVE-1 receptor.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20hyaluronan+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NIR%20hyaluronan%20AND+human)]

No publication is currently available.

## NIH Support

R01 CA112679

## References

1 Clement O., Luciani A. (2004). Imaging the lymphatic system: possibilities and clinical applications. Eur Radiol.
2 Styblo T., Aarsvold J.N., Grant S.F., Cohen C., Larsen T., Waldrop S., Alazraki N.P. (2001). Sentinel lymph nodes: optimizing success. Semin Roentgenol.
3 Hoh C.K., Wallace A.M., Vera D.R. (2003). Preclinical studies of [(99m)Tc]DTPA-mannosyl-dextran. Nucl Med Biol.
4 Salem C.E., Hoh C.K., Wallace A.M., Vera D.R. (2006). A preclinical study of prostate sentinel lymph node mapping with [99mTC]diethylenetetramine pentaacetic acid-mannosyl-dextran. J Urol.
5 Vera D.R., Wallace A.M., Hoh C.K., Mattrey R.F. (2001). A synthetic macromolecule for sentinel node detection: (99m)Tc-DTPA-mannosyl-dextran. J Nucl Med.
6 Torabi M., Aquino S.L., Harisinghani M.G. (2004). Current concepts in lymph node imaging. J Nucl Med.
7 Schoder H., Glass E.C., Pecking A.P., Harness J.K., Wallace A.M., Hirnle P., Alberini J.L., Vilain D., Larson S.M., Hoh C.K., Vera D.R. (2006). Molecular targeting of the lymphovascular system for imaging and therapy. Cancer Metastasis Rev.
8 Luciani A., Itti E., Rahmouni A., Meignan M., Clement O. (2006). Lymph node imaging: basic principles. Eur J Radiol.
9 Wunderbaldinger P. (2006). Problems and prospects of modern lymph node imaging. Eur J Radiol.
10 Qian C.N., Berghuis B., Tsarfaty G., Bruch M., Kort E.J., Ditlev J., Tsarfaty I., Hudson E., Jackson D.G., Petillo D., Chen J., Resau J.H., Teh B.T. (2006). Preparing the "soil": the primary tumor induces vasculature reorganization in the sentinel lymph node before the arrival of metastatic cancer cells. Cancer Res.
11 Harrell M.I., Iritani B.M., Ruddell A. (2007). Tumor-induced sentinel lymph node lymphangiogenesis and increased lymph flow precede melanoma metastasis. Am J Pathol.
12 Dadras S.S., Lange-Asschenfeldt B., Velasco P., Nguyen L., Vora A., Muzikansky A., Jahnke K., Hauschild A., Hirakawa S., Mihm M.C., Detmar M. (2005). Tumor lymphangiogenesis predicts melanoma metastasis to sentinel lymph nodes. Mod Pathol.
13 Van den Eynden G.G., Vandenberghe M.K., van Dam P.J., Colpaert C.G., van Dam P., Dirix L.Y., Vermeulen P.B., Van Marck E.A. (2007). Increased sentinel lymph node lymphangiogenesis is associated with nonsentinel axillary lymph node involvement in breast cancer patients with a positive sentinel node. Clin Cancer Res.
14 Jiang D., Liang J., Noble P.W. (2011). Hyaluronan as an immune regulator in human diseases. Physiol Rev.
15 Sironen R.K., Tammi M., Tammi R., Auvinen P.K., Anttila M., Kosma V.M. (2011). Hyaluronan in human malignancies. Exp Cell Res.
16 Aruffo A., Stamenkovic I., Melnick M., Underhill C.B., Seed B. (1990). CD44 is the principal cell surface receptor for hyaluronate. Cell.
17 Sakka S.G. (2007). Indocyanine green plasma disappearance rate as an indicator of hepato-splanchnic ischemia during abdominal compartment syndrome. Anesth Analg.
18 Sharma R., Wang W., Rasmussen J.C., Joshi A., Houston J.P., Adams K.E., Cameron A., Ke S., Kwon S., Mawad M.E., Sevick-Muraca E.M. (2007). Quantitative imaging of lymph function. Am J Physiol Heart Circ Physiol.